# IR-783-Glucosamine

Chemical name: | IR-783-Glucosamine
Abbreviated name: | IR-2
Synonym:
Backbone: | Compound
Target: | Lysosomes
Mechanism: | Unknown
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | IR-783
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20glucosamine)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low fluorescence background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals (4, 5).

Lysosomes are membranous vesicles found in most mammalian cells (6). Lysosomes contain various types of proteases, which have been implicated in migration, invasion, and metastasis of malignant cancer cells by the degradation of extracellular matrix (7). Glucosamine is used to synthesize highly glycosylated lysosomal proteins (8). The sizes of lysosomes are found to be larger in malignant cancer cells than in benign cancer cells (9). Carbocyanine IR-783 was conjugated to glucosamine for imaging lysosomal content in tumors with NIR fluorescence (10, 11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20glucosamine+Synthesis)]

The hydroxyl group in the 6-position of glucosamine was first converted to a primary amine, which was reacted with 3-(4-iodobutoxy)-phenyl acetate (10, 11). IR783 was conjugated to the phenol moiety of the linker of the resulting glucosamine to produce IR-783-glucosamine (IR-2). IR-2 has an extinction of coefficient of 157,000 M^-1^cm^-1^ and a quantum yield of 0.11, with a maximal excitation wavelength of 768 nm and a maximal emission wavelength of 784 nm in saline. The fluorescence intensities at pH 3–5 were higher than those at pH 6.4–7.2.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20glucosamine+In+Vitro)]

IR-2 at concentrations up to 0.5 mM exhibited minimal cytotoxicity in four human breast cancer cell lines: MCF-12A, MCF-7, MDA-MB-231, and MDA-MB-435 (10, 11). High fluorescence intensity was observed in small intracellular vesicles with a partially punctuated pattern at 24 h of incubation, most likely as a result of lysosomal localization. IR-2 was colocalized with a lysosomal marker, dextran, and a lysosomal glycoprotein, CD63. No such pattern was observed with IR-783. The IR-2 staining was not affected by either 5 mM glucosamine or 50 mM D-glucose.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20glucosamine+Rodentia)]

Li et al. (11) performed a preliminary study of IR-2 (100 nmol/mouse) in nude mice (n = 3) bearing MDA-MB-231, MDA-MB435, or MCF-7 tumors (200–300 mm^3^ in volume) using a whole-body fluorescence detection system. IR-2 showed a higher fluorescence signal in the tumors than IR-783 at 1–24 h after injection. The maximum IR-2 fluorescence intensities were 9.5, 7.5, and 3.0 × 10^11^ p/s/cm^2^/sr for MDA-MB-231, MDA-MB435, and MCF-7, respectively. On the other hand, the maximum IR-783 fluorescence intensities were 4.5, 2.0, and 1.0 × 10^11^ p/s/cm^2^/sr for MDA-MB-231, MDA-MB435, and MCF-7, respectively. The tumor/muscle ratios in all three tumors were ~3 and ~1 for IR-2 and IR-786 at most time points after injection, respectively. Biodistribution studies showed that the liver, kidneys, and intestines also displayed higher fluorescence intensities than the tumors at 24 h after injection. The muscle, brain, spleen, and blood contain little accumulation of IR-2. Tumor uptakes of IR-2 were three-fold higher than that of IR-783. IR-2 exhibited higher co-localization coefficients of CD63 in the three tumors than IR-783.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20glucosamine+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20glucosamine+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20glucosamine+human)]

No publication is currently available.

## NIH Support

CA112216, CA103175

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Robeson W., Dhawan V., Belakhlef A., Ma Y., Pillai V., Chaly T., Margouleff C., Bjelke D., Eidelberg D. (2003). Dosimetry of the dopamine transporter radioligand 18F-FPCIT in human subjects. J Nucl Med.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 de Duve C. (2005). The lysosome turns fifty. Nat Cell Biol.
7 Mignatti P., Rifkin D.B. (1993). Biology and biochemistry of proteinases in tumor invasion. Physiol Rev.
8 Glunde K., Guggino S.E., Ichikawa Y., Bhujwalla Z.M. (2003). A novel method of imaging lysosomes in living human mammary epithelial cells. Mol Imaging.
9 Glunde K., Guggino S.E., Solaiyappan M., Pathak A.P., Ichikawa Y., Bhujwalla Z.M. (2003). Extracellular acidification alters lysosomal trafficking in human breast cancer cells. Neoplasia.
10 Li C., Greenwood T.R., Bhujwalla Z.M., Glunde K. (2006). Synthesis and characterization of glucosamine-bound near-infrared probes for optical imaging. Org Lett.
11 Li C., Greenwood T.R., Glunde K. (2008). Glucosamine-bound near-infrared fluorescent probes with lysosomal specificity for breast tumor imaging. Neoplasia.